# ^125^I-Labeled mesenchymal-epithelial transition factor binding peptide-8-aminooctanoic acid

Chemical name: | ^125^I-Labeled mesenchymal-epithelial transition factor binding peptide-8-aminooctanoic acid | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-aminooctanoic acid-Cys
Abbreviated name: | [^125^I]cMBP-AOC | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-aminooctanoic acid-Cys
Synonym: | | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-aminooctanoic acid-Cys
Agent Category: | Ligand | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-aminooctanoic acid-Cys
Target: | Mesenchymal-epithelial transition factor receptor (c-Met); hepatocyte growth factor receptor (HGFR) | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-aminooctanoic acid-Cys
Target Category: | Receptor | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-aminooctanoic acid-Cys
Method of detection: | Single photon-emission computed tomography (SPECT); gamma planar imaging | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-aminooctanoic acid-Cys
Source of signal / contrast: | ^125^I | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-aminooctanoic acid-Cys
Activation: | No | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-aminooctanoic acid-Cys
Studies: | - In vitro; - Rodents | Structure of cMBP-AOC.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cMBP-GGG-Cy5.5)]

The hepatocyte growth factor (HGF) is the only known ligand of the mesenchymal-epithelial transition factor (c-Met) (also known as the HGF receptor) that has an important function, including cell development, proliferation, scattering, migration, and angiogenesis, all of which are necessary for the survival and repair of tissues (1). c-Met is known to mediate its activity through an intracellular tyrosine kinase (TK) that activates different signal transduction pathways leading to initiation of the various cell processes (2). Also, deregulation of c-Met activity due to paracrine/autocrine activation, overexpression, or a mutation promotes the development of a neoplastic cell phenotype (2). Overexpression of c-Met and HGF has been associated with a poor prognosis and survival of the patient (3), suggesting that the c-Met receptor may be a suitable target for the detection of cancers at an early stage, which could help in the development of an appropriate treatment regimen to improve patient prognosis (4). c-Met is the target of several drugs under evaluation in clinical trials (http://clinicaltrials.gov/ct2/results?term=HGFR) approved by the United States Food and Drug Administration. Investigators recently generated a monoclonal antibody (mAb) that inhibits the HGF–c-Met interaction and identified the active mAb epitope peptide as KSLSRHDHIHHH, which was designated as the c-Met binding peptide (cMBP) (5). The cMBP and its derivatives (containing a tri-amino acid linker, Gly-Gly-Gly (GGG), or an aliphatic carbon linker, 8-aminooctanoic acid (AOC)) were labeled with ^125^I to generate ^125^I-cMBP, 1^25^I-cMBP-GGG, and ^125^I-cMBP-AOC, and these agents were used to detect c-Met TK-positive tumor xenografts in mice (6). From this study the investigators concluded that although ^125^I-cMBP-GGG was suitable for the imaging of c-Met TK expressing tumors, the signal to background obtained from this nuclide was not very strong, and the results could probably be improved by using another radionuclide and/or by modifying the linkers.

In an attempt to generate a c-Met–positive tumor imaging agent superior to ^125^I-cMBP, ^125^I-cMBP-GGG, and ^125^I-cMBP-AOC, investigators conjugated a near-infrared (NIR) fluorescent dye, cyanine 5.5 (Cy5.5), to cMBP-GGG and cMBP-AOC to obtain cMBP-GGG-Cy5.5 and cMBP-AOC-Cy5.5 (4). The Cy5.5-conjugated cMBP derivatives were then evaluated for the NIR imaging of c-Met–positive xenograft tumors in a mouse model.

This chapter describes the in vitro and in vivo characterization of only ^125^I-cMBP-AOC, where the radionuclide is the same, but the linker was changed. The other c-Met imaging agents (1^25^I-cMBP, ^125^I-cMBP-GGG, cMBP-GGG-Cy5.5, and cMBP-AOC-Cy5.5) are described in separate MICAD chapters (7-10).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20synthesis)]

The synthesis of cMBP was described previously (4). Briefly, the cMBP-AOC peptide was synthesized using Fmoc chemistry, with a purity of 90%. The AOC linker was bound on the C-trminal of cMBP. The ^125^I labeling of cMBP-AOC was done by the chloramine T method, and the reaction was terminated with sodium bisulfite. The radiochemical purity of the labeled compound was reported to be between 90% and 95% at 24 h after the labeling as determined with instant thin-layer chromatography (ITLC). The stability of ^125^I-cMBP-AOC in human serum was reported to be 90% at 1 h and 88% at 4 h as determined with ITLC.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed]

Using human glioblastoma U87MG cells, the 50% inhibitory concentration of cMBP-AOC was determined to be 85.3 nM (6). In a blocking study, the cells were exposed to ^125^I-cMBP-AOC (2 pmol) in the presence of excess unlabeled cMBP-AOC (1 nmol), and a significant (P = 0.001) reduction in cellular binding of the radiochemical was observed compared with the controls (6). Also, a peptide containing amino acids similar to the cMBP, but in a scrambled order, had no effect on the binding of ^125^I-cMBP to the cells. A high internalization of ^125^I-cMBP-AOC by the cells was reported (6).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cMBP-GGG-Cy5.5+rodentia)]

The biodistribution of ^125^I-cMBP-AOC was studied in mice (n = 5 animals/time point) bearing U87MG cell xenograft tumors (6). The animals were injected with the radiochemical through the tail vein and euthanized at predetermined time points from 30 min to 24 h after the treatment. Tissues and organs of interest were subsequently removed from the animals; accumulated radioactivity was measured with a gamma counter, and the accumulated radioactivity data was presented as percent of injected dose per gram tissue (% ID/g). A high uptake of radioactivity by the pancreas was reported (18.41 ± 0.74% ID/g at 30 min, 36.53 ± 5.14% ID/g at 4 h, and 0.12 ± 0.04% ID/g at 24 h). A high accumulation of the label in the kidneys was also observed (20.17 ± 3.73% ID/g at 30 min, 5.24 ± 2.41% ID/g at 4 h, and 0.17 ± 0.006% ID/g at 24 h). The tumor uptake was 5.24 ± 0.66% ID/g at 30 min and decreased to 0.04 ± 0.02% ID/g by 24 h.All other organs showed a similar distribution of radioactivity at the different time points (for details please see Table 1 of Kim, Park, et al. (6). In the same study, by comparison, the biodistribution of 125I-cMBP in the pancreas, kidneys and the tumor was 47.28 ± 4.39, 17.18 ± 1.12 and 9.3 ± 0.78%ID/g at 30 min after administration. The tumor/blood ratio with ^125^I-cMBP-AOC was reported to be 1.78 at 4 h after treatment. Because of the high uptake of ^125^I-cMBP-AOC by the pancreas, the expression of c-Met in this organ was investigated with reverse-transcriptase polymerase chain reaction. A low expression of c-Met was observed in the pancreas, indicating that the uptake of ^125^I-cMBP-AOC by this organ was not c-Met–mediated, and accumulation of label in this organ was non-specific. No blocking studies were reported.

From these studies, the investigators concluded that although ^125^I-cMBP-AOC was taken up by c-Met–expressing tumors, it was similar to the biodistribution of cMBP and therefore not a suitable imaging agent because it generated a high background due to accumulation in other tissue and organs of the animals (6).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cMBP-GGG-Cy5.5+Non-Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cMBP-GGG-Cy5.5+Non-Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cMBP-GGG-Cy5.5+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimer]

No information is currently available.

## References

1 Naran S., Zhang X., Hughes S.J. (2009). Inhibition of HGF/MET as therapy for malignancy. Expert Opin Ther Targets.
2 Abounader R., Laterra J. (2005). Scatter factor/hepatocyte growth factor in brain tumor growth and angiogenesis. Neuro Oncol.
3 Birchmeier C., Birchmeier W., Gherardi E., Vande Woude G.F. (2003). Met, metastasis, motility and more. Nat Rev Mol Cell Biol.
4 Kim E.M., Park E.H., Cheong S.J., Lee C.M., Jeong H.J., Kim D.W., Lim S.T., Sohn M.H. (2009). In vivo imaging of mesenchymal-epithelial transition factor (c-Met) expression using an optical imaging system. Bioconjug Chem.
5 Kim K., Hur Y., Ryu E.K., Rhim J.H., Choi C.Y., Baek C.M., Lee J.H., Chung J. (2007). A neutralizable epitope is induced on HGF upon its interaction with its receptor cMet. Biochem Biophys Res Commun.
6 Kim E.M., Park E.H., Cheong S.J., Lee C.M., Kim D.W., Jeong H.J., Lim S.T., Sohn M.H., Kim K., Chung J. (2009). Characterization, biodistribution and small-animal SPECT of I-125-labeled c-Met binding peptide in mice bearing c-Met receptor tyrosine kinase-positive tumor xenografts. Nucl Med Biol.
7 Chopra, A., 125I labeled mesenchymal-epithelial transition factor binding peptide [125I-cMBP]. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
8 Chopra, A., 125I labeled mesenchymal-epithelial transition factor binding peptide-Gly-Gly-Gly. [125I-cMBP-GGG]. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
9 Chopra, A., Mesenchymal-epithelial transition factor binding peptide-Gly-Gly-Gly-conjugated to Cy5.5 [cMBP-GGG-Cy5.5]. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
10 Chopra, A., Mesenchymal-epithelial transition factor binding peptide with an 8-aminooctanoic acid linker conjugated to Cy5.5. [cMBP-AOC-Cy5.5]. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.